# N,N-Diethyl-2-2(2-(4-[^11^C]methoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide

Chemical name: | N,N-Diethyl-2-2(2-(4-[^11^C]methoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide
Abbreviated name: | [^11^C]DPA-713
Synonym:
Agent Category: | Compound
Target: | Peripheral benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target Category: | Receptor
Method of detection: | PET
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713)]

Benzodiazepines are used for their sedative, anxiolytic, and muscle-relaxant properties (1). Their mechanism of action involves the binding of a ligand to a specific benzodiazepine receptor. Two types of benzodiazepine receptors have been identified: a central receptor and a peripheral one. The central benzodiazepine receptor (CBR) is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (2). The peripheral benzodiazepine receptor (PBR), first thought to be a subtype of the CBR, was later identified as a separate class of receptor with its own structure, physiologic functions, and location on the outer membrane of the mitochondria (3).

The PBR structure consists of a trimeric complex with an adenine nucleotide carrier and a voltage-dependent anion that form the mitochondrial permeability transition pore (3). Although it has been shown to be involved in numerous biological processes, the physiologic role of the PBR is still unclear (4). PBR is abundant in peripheral organs such as the kidneys, lungs, and heart, whereas lower levels are found in the brain (5). A significant increase in PBR expression after neural injury or inflammation (e.g., Alzheimer's disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy) has been observed and has been associated with microglial activation (6, 7).

The development of PBR radioligands for positron emission tomography (PET) has enabled the study of microglial activation in the brain (8). One of these radioligands, 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), was developed as a probe for studying the function and expression of PBR (9). Unfortunately, [^11^C]PK11195 displays a poor signal-to-noise ratio and low brain permeability, which decreases its sensitivity for detecting areas of microglia activation.

Other ligands displaying better brain kinetics have recently been synthesized and studied. Among them, N,N-diethyl-2-2(2-(4-[^11^C]methoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide ([^11^C]DPA-713), a compound from the family of pyrazolopyrimidines (10), has shown a slightly higher affinity (K_i_ = 4.7 nM) for PBR than does [^11^C]PK11195 (K_i_ = 9.3 nM). [^11^C]DPA-713 is substantially more selective for the PBR than for the CBR (K_i_ > 10,000 nM for the CBR).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610)
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20synthesis)]

[^11^C]DPA-713 can be prepared by O-alkylation of the phenolic derivative N,N-diethyl-2-[2-(4-hydroxyphenyl)-5,7-dimethylpyrazolo[1,5-a]pyrimidin-3-yl]-acetamide with [^11^C]methyl iodide ([^11^C]MeI), as described by James et al. (11). The radiochemical yield of [^11^C]DPA-713 was 9% (non-decay-corrected) with a radiochemical purity >98%. The specific activity of the radioligand measured at the end of the synthesis was 36 GBq/µmol (973 mCi/µmol), and the total time of synthesis was about 13 min.

In 2006, Thominiaux et al. (12) reported another radiosynthesis method using [^11^C]methyl triflate ([^11^C]MeOTf) instead of [^11^C]MeI. Their method gave an improved yield (30-38%) compared with [^11^C]MeI, and used a simpler purification method (with HPLC)). Briefly, [^11^C]MeOTf was bubbled through 0.3-0.5 mg of DPA-713 dissolved in acetone (300 µl) and aqueous NaOH (12 µmol, 3 N), at –10 °C (in an ethanol-ice bath). After trapping of [^11^C]MeOTf for about 3 min, the reaction mixture was concentrated to dryness at 110 °C, cooled, diluted with 0.6 ml of the HPLC mobile phase, and injected onto the HPLC column. This last step enabled separation of the radioligand from its unlabeled precursor.

Log P (P = octanol-water partition coefficient) for [^11^C]DPA-713 was found to be 2.4 (11), which is within the optimum range (2 to 3) for achieving high brain uptake with weak nonspecific binding (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20in%20vitro)]

PBR binding affinities of DPA-713, DPA-714 and PK1195 were assessed with competitive binding with [^3^H]PK11195 in rat kidney membranes with K_i_ values of 7.0 ± 0.4, 4.7 ± 0.2, and 9.3 ± 0.5 nm, respectively (10, 11, 14). The three compounds exhibited K_i_ values of > 10, 000 nM for CBR. DPA-713 did not stimulate pregnenolone synthesis in a standard steroidogenic assay, whereas DPA-714 and PK1195 increase pregnenolone synthesis by 80% and 60%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20rodentia%5BMeSH%5D)]

Boutin et al. (15) performed PET imaging in rats (n = 4-5/group) with neuroinflammation induced with alpha-amino-3-hydroxy-5-methyl-4-isoxazolepropionate in the brain. Binding potential values for [^11^C]DPA-713 was significantly higher than that of [^11^C]PK11195 (1.57 ± 0.36 versus 0.66 ± 0.15; P < 0.05). Displacement studies were performed by injection of 1 mg/kg of DPA-713 or PK11195 at 20 min after injection of [^11^C]DPA-713. Rapid displacement of radioactivity in the brain lesion site was observed with both unlabeled compounds with complete displacement within 15 min after injection of unlabeled compounds. No change in radioactivity was observed in the contralateral side.

Doorduin et al. (16) performed PET imaging in rats (n = 4-5/group) with Herpes encephalitis. Accumulation of [^11^C]DPA-713 in the infected brain areas was comparable to that of [^11^C]PK11195, but [^11^C]PA-713 showed lower non-specific binding. The radioactivity levels in the infected brain areas were about 1-fold higher than the control brain areas. Pretreatment with 5 mg/kg PK11195 significantly reduced the accumulation in the infected brain areas to background levels (P < 0.05). Ex vivo biodistribution studies showed that the infected brain areas with specific accumulation were the bulbus olfactorius, hippocampus, medulla, and pons. The lung exhibited a high specific binding for [^11^C]PA-713 in the infected animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20%28dog%20OR%20rabbit%20OR%20sheep%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20%28%28primate%20NOT%20human%29%20OR%20baboon%29)]

James et al. (11) evaluated the uptake of [^11^C]DPA-713, using dynamic PET brain scans of 13-year-old Papio hamadryas baboons (~26.5 kg each) injected with 200 MBq (5.4 mCi) of the radiotracer. Data were acquired every 2 min for a total time period of 60 min post injection. Maximal accumulation of ~0.006% of injected dose (ID)/ml was reached at 20 min post injection and stayed approximately constant for the remaining 40 min of the imaging procedure. To assess the in vivo specificity and selectivity of [^11^C]DPA-713, two blocking studies were performed 3 weeks apart, in which either flumazenil (a CBR-specific ligand) or PK11195 (a PBR-specific ligand) was injected intravenously into the baboons 5 min before they received the radiotracer. It was observed that the pretreatment with PK11195 (5 mg/kg) significantly decreased the accumulation of [^11^C]DPA-713 compared with the baseline study described above. The measured values for brain activity (in % ID/ml) were as follows: 0.007 at ~2 min post injection, 0.0035 at 10 min, 0.0035 at 20 min, and 0.002 at 60 min. In contrast, pretreatment with flumazenil (1 mg/kg) showed no inhibitory effect on the uptake of [^11^C]DPA-713. In that case, the brain activity pattern was not significantly different from the pattern obtained with no-carrier-added [^11^C]DPA-713. A maximum uptake of almost 0.006% ID/ml was reached at 20 min post injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPA-713%20AND%20human)]

Endres et al. (17) reported on PET studies in 7 healthy volunteers after injection of 689 MBq (18.6 mCi) of [^11^C]DPA-713 or 681 MBq (18.4 mCi) of [^11^C]PK11195. Tracer uptake was evaluated for the cerebellum, frontal cortex, white matter, and pons with a preference for the 2-tissue model over the 1-tissue model. The radioactivity of [^11^C]DPA-713 in the brain regions was 2-3 folds greater that of [^11^C]PK11195. The volume of distribution values for [^11^C]DPA-713 (3.08-5.06) were >10-folds than those for [^11^C]PK11195 (0.25-0.42). Accumulation in the lung was high up to 10 min post injection. The radioactivity in the myocardium became detectable at 2 min. The radioactivity in the heart decreased for 20 min and remained constant at 75 min. Injection of excess unlabeled PK11195 (650 nmol/kg) 30 min after [^11^C]PK11195 (0.94 nmol/kg) led to a rapid decrease (48%) in the radioactivity in the myocardium.

## References

1 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
2 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
3 Casellas P., Galiegue S., Basile A.S. (2002). Peripheral benzodiazepine receptors and mitochondrial function. Neurochem Int.
4 Papadopoulos V. (2004). In search of the function of the peripheral-type benzodiazepine receptor. Endocr Res.
5 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
6 Wilms H., Claasen J., Rohl C., Sievers J., Deuschl G., Lucius R. (2003). Involvement of benzodiazepine receptors in neuroinflammatory and neurodegenerative diseases: evidence from activated microglial cells in vitro. Neurobiol Dis.
7 Decaudin D. (2004). Peripheral benzodiazepine receptor and its clinical targeting. Anticancer Drugs.
8 Kassiou M., Meikle S.R., Banati R.B. (2005). Ligands for peripheral benzodiazepine binding sites in glial cells. Brain Res Brain Res Rev.
9 Kropholler M.A., Boellaard R., Schuitemaker A., van Berckel B.N., Luurtsema G., Windhorst A.D., Lammertsma A.A. (2005). Development of a tracer kinetic plasma input model for (R)-[11C]PK11195 brain studies. J Cereb Blood Flow Metab.
10 Selleri S., Bruni F., Costagli C., Costanzo A., Guerrini G., Ciciani G., Costa B., Martini C. (2001). 2-Arylpyrazolo[1,5-a]pyrimidin-3-yl acetamides. New potent and selective peripheral benzodiazepine receptor ligands. Bioorg Med Chem.
11 James M.L., Fulton R.R., Henderson D.J., Eberl S., Meikle S.R., Thomson S., Allan R.D., Dolle F., Fulham M.J., Kassiou M. (2005). Synthesis and in vivo evaluation of a novel peripheral benzodiazepine receptor PET radioligand. Bioorg Med Chem.
12 Thominiaux C., Dolle F., James M.L., Bramoulle Y., Boutin H., Besret L., Gregoire M.C., Valette H., Bottlaender M., Tavitian B., Hantraye P., Selleri S., Kassiou M. (2006). Improved synthesis of the peripheral benzodiazepine receptor ligand [(11)C]DPA-713 using [(11)C]methyl triflate. Appl Radiat Isot.
13 Halldin C., Gulyas B., Langer O., Farde L. (2001). Brain radioligands--state of the art and new trends. Q J Nucl Med.
14 James M.L., Fulton R.R., Vercoullie J., Henderson D.J., Garreau L., Chalon S., Dolle F., Costa B., Guilloteau D., Kassiou M. (2008). DPA-714, a new translocator protein-specific ligand: synthesis, radiofluorination, and pharmacologic characterization. J Nucl Med.
15 Boutin H., Chauveau F., Thominiaux C., Gregoire M.C., James M.L., Trebossen R., Hantraye P., Dolle F., Tavitian B., Kassiou M. (2007). 11C-DPA-713: a novel peripheral benzodiazepine receptor PET ligand for in vivo imaging of neuroinflammation. J Nucl Med.
16 Doorduin J., Klein H.C., Dierckx R.A., James M., Kassiou M., de Vries E.F. (2009). [11C]-DPA-713 and [18F]-DPA-714 as new PET tracers for TSPO: a comparison with [11C]-(R)-PK11195 in a rat model of herpes encephalitis. Mol Imaging Biol.
17 Endres C.J., Pomper M.G., James M., Uzuner O., Hammoud D.A., Watkins C.C., Reynolds A., Hilton J., Dannals R.F., Kassiou M. (2009). Initial evaluation of 11C-DPA-713, a novel TSPO PET ligand, in humans. J Nucl Med.